# [4-O-methyl-^11^C]-8-[(E)-2-(3,4-Dimethoxyphenyl)ethenyl]-1,3-diethyl-7-methylpurine-2,6-dione

Chemical name: | [4-O-methyl-^11^C]-8-[(E)-2-(3,4-Dimethoxyphenyl)ethenyl]-1,3-diethyl-7-methylpurine-2,6-dione
Abbreviated name: | [^11^C]KW-6002
Synonym:
Agent Category: | Compound
Target: | Adenosine A_2A_ receptor
Target Category: | Receptor-ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KW-6002)]

Adenosine is an endogenous nucleoside that modulates a number of physiological functions in the central nervous system and in peripheral organs, such as the heart, kidneys, and muscle (1, 2). The effect is mediated by two major subtypes of receptors (A_1_ and A_2A_) and two minor subtypes (A_2B_ and A_3_). In the central nervous system, A_1_ receptors are present both pre- and postsynaptically in the hippocampus, cerebral cortex, thalamus, striatum, and cerebellum. A_2A_ receptors are highly concentrated and co-localized with dopamine D_1_ and D_2_ receptors in the striatum, nucleus accumbens, and olfactory tubercle. A_2A_ receptors are also present in low amounts in the hippocampus and cortex. A_2B_ receptors are widely distributed, but concentrations are high in the gastrointestinal tract. A_3_ receptors are also widely distributed, with high concentrations in testis. A_1_ and A_3_ receptors mediate inhibition of adenylyl cyclase, whereas A_2A_ and A_2B_ receptors mediate stimulation. Changes in the adenosine functions are implicated in epilepsy, ischemic cerebral stroke, movement disorders, sleep disorders, and psychiatric disorders (3-5).

A_2A_ receptors have been studied in vivo with positron emission tomography (PET) using [7-methyl-^11^C]-(E)-8-(3,4,5-trimethoxystyryl)-1,3,7-trimethylxanthine ([^11^C]TMSX), a methyl xanthine analog of KF17387 with selective A_2A_ antagonistic activity (6). [^11^C]TMSX is being developed as a PET agent for the non-invasive study of A_2A_ receptors in the human brain. 8-[(E)-2-(3,4-Dimethoxyphenyl)ethenyl]-1,3-diethyl-7-methylpurine-2,6-dione (KW-6002), another xanthine derivative, is a potent and selective A_2A_ antagonist with a 50% inhibition concentration (K_i_) value of 2.2 nM (7). [4-O-methyl-^11^C]-KW-6002 ([^11^C]KW-6002) is being developed as a PET agent for the non-invasive study of A_2A_ receptors in the human brain (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+KW-6002%20and%20synthesis)]

Hirani et al. (7) reported that [^11^C]KW-6002 was synthesized by alkylation of the O-desmethyl precursor with [^11^C]methyl iodide in the presence of NaOH for 6 min at 100ºC. Purification with high-performance liquid chromatography provided radiochemical purity of >94%. Specific activity was 17 ± 11 GBq/μmol (0.46 ± 0.30 Ci/μmol) at time of injection for biodistribution studies. The radiochemical yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KW-6002%20and%20in%20vitro)]

The K_i_ values of KW-6002 for rat striatal A_2A_ and forebrain A_1_ receptors were 2.2 and 150 nM, respectively (7). The K_i_ value of KW-6002 for human striatal A_2A_ receptors was 12 nM with >800-fold selectivity for the human A_1_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20KW-6002%20and%20rodentia)]

Biodistribution studies in normal rats showed a high accumulation of radioactivity in the heart ventricle (5.3 uptake units = (cpm/g tissue)/(injected cpm/g body weight)), followed by the kidney (2.8 uptake units), liver (2.0 uptake units), muscle (1.6 uptake units), and testis (1.5 uptake units) at 75 min after injection of [^11^C]KW-6002 (7). The level of radioactivity was low in the blood (0.2 uptake units). In the brain, the striatum (3.3 uptake units) exhibited the highest radioactivity, whereas the cortex (1.7 uptake units) had the lowest accumulation. The striatum/cortex ratio was ~2. There was high binding in other regions, including the cerebellum (3.0 uptake units). Pretreatment with KW-6002 (1 mg/kg) reduced the binding in all brain regions by >75%. In the peripheral tissues, KW-6002 reduced binding in the heart, kidney, skeletal muscle, and testis. Binding in the brain regions was blocked by KW-6002 but not by KF15373 (A_1_ antagonist) or MRS 1745 (A_2B_ antagonist). The homogenates of the striatum and cerebellum contained >87% intact [^11^C]KW-6002 at 30 and 60 min after injection. PET scanning with [^11^C]KW-6002 demonstrated a specific signal (binding potential (BP)) in the striatum that could be estimated using compartmental modeling with the cortex as the reference region input function. Specific binding was, however, also detected in extrastriatal regions, including brain areas (cerebellum and thalamus) reported to have low adenosine A_2A_ receptor density. The striatal BP (0.30) was reduced by KW-6002 (0.03) but not by KF15373 (0.31). It indicates subtype specific binding to A_2A_, but not to A_1_.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20KW-6002%20and%20%28dog%20or%20or%20rabbit%20or%20sheep%20or%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20KW-6002%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20KW-6002%20and%20human)]

Brooks et al. (8) reported on PET studies in 15 healthy volunteers who each received an injection of 289 MBq (7.8 mCi) [^11^C]KW-6002. In a two-tissue compartmental model with a blood volume component, the caudate (3.38) exhibited the highest BP, followed by the putamen (2.90), accumbens (2.37), cerebellum (2.26), and thalamus (2.19). The binding in these five regions was blocked by oral doses of KW-6002 administered daily for 14 d before tracer injection with the half-saturation oral dose of 0.62 mg (estimated from volumes of distribution). Internal dosimetry data for [^11^C]TMSX in humans are not available in the literature.

## References

1 Fredholm B.B., Abbracchio M.P., Burnstock G., Daly J.W., Harden T.K., Jacobson K.A., Leff P., Williams M. (1994). Nomenclature and classification of purinoceptors. Pharmacol Rev.
2 Palmer T.M., Stiles G.L. (1995). Adenosine receptors. Neuropharmacology.
3 Dunwiddie T.V., Masino S.A. (2001). The role and regulation of adenosine in the central nervous system. Annu Rev Neurosci.
4 El Yacoubi M. Costentin J. Vaugeois J.M. Adenosine A2A receptors and depression Neurology 2003 61Suppl 611 S82 7 14663017
5 von Lubitz D.K. (2001). Adenosine in the treatment of stroke: yes, maybe, or absolutely not?. Expert Opin Investig Drugs.
6 Noguchi J., Ishiwata K., Wakabayashi S., Nariai T., Shumiya S., Ishii S., Toyama H., Endo K., Suzuki F., Senda M. (1998). Evaluation of carbon-11-labeled KF17837: a potential CNS adenosine A2a receptor ligand. J Nucl Med.
7 Hirani E., Gillies J., Karasawa A., Shimada J., Kase H., Opacka-Juffry J., Osman S., Luthra S.K., Hume S.P., Brooks D.J. (2001). Evaluation of [4-O-methyl-(11)C]KW-6002 as a potential PET ligand for mapping central adenosine A(2A) receptors in rats. Synapse.
8 Brooks D.J., Doder M., Osman S., Luthra S.K., Hirani E., Hume S., Kase H., Kilborn J., Martindill S., Mori A. (2008). Positron emission tomography analysis of [(11)C]KW-6002 binding to human and rat adenosine A(2A) receptors in the brain. Synapse.